# 2-{4-[-Pyridin-4-yl-1-(2-[^18^F]fluoro-ethyl)-1H-pyrazol-3-yl]-phenoxymethyl}-quinoline

Chemical name: | 2-{4-[-Pyridin-4-yl-1-(2-[^18^F]fluoro-ethyl)-1H-pyrazol-3-yl]-phenoxymethyl}-quinoline
Abbreviated name: | [^18^F]JNJ41510417
Synonym:
Agent category: | Compound
Target: | Phosphodiesterase type 10A
Target category: | Enzyme binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=JNJ41510417)]

Phosphodiesterases (PDEs) are composed of at least 11 families of enzymes that hydrolyze cyclic 3´,5´-adenosine monophosphate (cAMP) and/or cyclic 3´,5´-guanosine monophosphate (cGMP) to the corresponding inactive 5´-AMP and 5´-GMP, respectively (1, 2). These second-messenger cyclic nucleotides are formed in response to stimuli (such as hormones, neurotransmitters, and cytokines) to regulate cellular functions. PDEs are essential in the termination of cellular responses via their degradation of cyclic nucleotides. PDE type-10A (PDE10A) is a dual-specificity PDE that can act on both cAMP and cGMP (3). PDE10A is found mainly in the brain (striatum) and testes, with low concentrations in other tissues (4). PDE10A may play a role in the regulation of glutamatergic and dopaminergic functions in neurons (5, 6). PDE10A inhibitors have been studied in the treatment of neuropsychiatric disorders such as schizophrenia, Huntington’s disease, Parkinson’s disease, obsessive-compulsive disorder, and addiction (7-11).

1-(3,4-Dimethoxybenzyl)-6,7-dimethoxyisoquinoline (papaverine) has been found to be a specific inhibitor of PDE10A with 50% inhibition concentration (IC_50_) values of 36 nM for PDE10A, 1,300 nM for PDE3A, and 320 nM for PDE4D (9). 1-(3-[^11^C]Methoxy-4-methoxybenzyl)-6,7-dimethoxyisoquinoline ([^11^C]Papaverine)has been evaluated as a positron emission tomography (12) agent for the non-invasive study of PDE10A in the brain in rats and monkeys (13). However, the results of these studies indicated that the rapid brain clearance of the tracer limits its utility as a PET agent for in vivo measurements of PDE10A. In this chapter, 2-{4-[-pyridin-4-yl-1-(2-[^18^F]fluoro-ethyl)-1H-pyrazol-3-yl]-phenoxymethyl}-quinoline ([^18^F]JNJ4151047) was found to be a selective inhibitor of PED10A (>1,000-fold better selectivity than the other nine PDE subtypes) with an IC_50_ value of 0.5 nM for PDE10A (14). [^18^F]JNJ4151047 has been evaluated in rats and PED10A-knockout mice for in vivo brain imaging of PED10A activity.

### Related Resource Links:

- Chapters in MICAD (PDE (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=PDE+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (PDE10A (http://www.ncbi.nlm.nih.gov/gene/10846))
- Articles in Online Mendelian Inheritance in Man (OMIM) (PDE10A (http://www.ncbi.nlm.nih.gov/omim/610652))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=JNJ41510417%20and%20synthesis)]

The synthesis of [^18^F]JNJ4151047 was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=JNJ41510417%20and%20in%20vitro)]

[^nat^F]JNJ4151047 was found to be a selective inhibitor of PED10A (>1,000-fold greater inhibition than PDE1B1, PDE2A, PDE3A, PDE4D3, PDE5A3, PDE6, PDE7A, PDE8A1, and PDE9A) with an IC_50_ value of 0.5 nM for rat PDE10A (14). [^nat^F]JNJ4151047 exhibited a measured log D_7.4_ lipophilicity value of 4.7.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=JNJ41510417%20and%20rodentia)]

Ex vivo biodistribution studies in normal rats (n = 3/group) showed high initial accumulation of radioactivity in the liver at 2 min after injection of [^18^F]JNJ4151047 (41.1% injected dose (ID)/g), followed by the intestines (9.4% ID/g), kidney (6.9% ID/g), and lung (2.4% ID/g) (14). [^18^F]JNJ4151047 accumulation in the brain was 0.447% ID/g at 5 min, 0.266% ID/g at 30 min, and 0.257% ID/g at 60 min after injection. Radioactivity in the liver, stomach, and intestines increased in the later time points, whereas other tissues showed rapid washout. The regional brain accumulation at 60 min after injection was highest in the striatum (2.6% ID/g) and lowest in the cerebellum (0.4% ID/g), as predicted by the density of PDE10A enzymes. The blood concentration was 0.3% ID/g. There was ~73% of intact [^18^F]JNJ4151047 in the plasma at 60 min after injection, with one major radioactive hydrophilic metabolite. In the brain, 95% of [^18^F]JNJ4151047 was intact at 30 min after injection. No blocking studies were performed.

Celen et al. (14) performed dynamic PET studies of the brain in normal rats with high radioactivity in the striatum and only background radioactivity in the cortex and cerebellum at 20–60 min after injection of [^18^F]JNJ4151047. A maximum striatum/cerebellum ratio of 2.9 was observed at 32 min after injection. Pretreatment (60 min) with PED10A inhibitors (TP-10 and MP-10, 5 mg/kg) or JNJ4151047 (2.5 mg/kg) reduced the striatum/cerebellum ratio to <1.4. A displacement study with MP-10 (3 mg/kg) at 32 min after [^18^F]JNJ4151047 injection reduced the striatum/cerebellum ratio to 1.0 at 60 min after injection. Imaging studies in PDE10A-knockout and wild-type mice exhibited a high uptake in the striatum of the wild-type mice but not in the knockout mice. Ex vivo autoradiography of brain sections showed that the radioactivity in the striatum of the wild-type mice at 75 min after injection was 22.5-fold higher than that in the striatum of the knockout mice at the same time point. Hence, there was specific accumulation of [^18^F]JNJ4151047 in the striatum.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=JNJ41510417%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=JNJ41510417%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=JNJ41510417%20and%20human)]

No publication is currently available.

## References

1 Sutherland E.W., Rall T.W. (1958). Fractionation and characterization of a cyclic adenine ribonucleotide formed by tissue particles. J Biol Chem.
2 Essayan D.M. (2001). Cyclic nucleotide phosphodiesterases. J Allergy Clin Immunol.
3 Fujishige K., Kotera J., Michibata H., Yuasa K., Takebayashi S., Okumura K., Omori K. (1999). Cloning and characterization of a novel human phosphodiesterase that hydrolyzes both cAMP and cGMP (PDE10A). J Biol Chem.
4 Fujishige K., Kotera J., Omori K. (1999). Striatum- and testis-specific phosphodiesterase PDE10A isolation and characterization of a rat PDE10A. Eur J Biochem.
5 Nishi A., Kuroiwa M., Shuto T. (2010). Role of phosphodiesterases in dopamine signal transduction. Nippon Yakurigaku Zasshi.
6 Xie Z., Adamowicz W.O., Eldred W.D., Jakowski A.B., Kleiman R.J., Morton D.G., Stephenson D.T., Strick C.A., Williams R.D., Menniti F.S. (2006). Cellular and subcellular localization of PDE10A, a striatum-enriched phosphodiesterase. Neuroscience.
7 Kehler J., Kilburn J.P. (2009). Patented PDE10A inhibitors: novel compounds since 2007. Expert Opin Ther Pat.
8 Chappie T., Humphrey J., Menniti F., Schmidt C. (2009). PDE10A inhibitors: an assessment of the current CNS drug discovery landscape. Curr Opin Drug Discov Devel.
9 Siuciak J.A. (2008). The role of phosphodiesterases in schizophrenia : therapeutic implications. CNS Drugs.
10 Menniti F.S., Chappie T.A., Humphrey J.M., Schmidt C.J. (2007). Phosphodiesterase 10A inhibitors: a novel approach to the treatment of the symptoms of schizophrenia. Curr Opin Investig Drugs.
11 Hebb A.L., Robertson H.A. (2007). Role of phosphodiesterases in neurological and psychiatric disease. Curr Opin Pharmacol.
12 Akerman M.E., Pilch J., Peters D., Ruoslahti E. (2005). Angiostatic peptides use plasma fibronectin to home to angiogenic vasculature. Proc Natl Acad Sci U S A.
13 Tu Z., Xu J., Jones L.A., Li S., Mach R.H. (2010). Carbon-11 labeled papaverine as a PET tracer for imaging PDE10A: radiosynthesis, in vitro and in vivo evaluation. Nucl Med Biol.
14 Celen S., Koole M., De Angelis M., Sannen I., Chitneni S.K., Alcazar J., Dedeurwaerdere S., Moechars D., Schmidt M., Verbruggen A., Langlois X., Van Laere K., Andres J.I., Bormans G. (2010). Preclinical evaluation of 18F-JNJ41510417 as a radioligand for PET imaging of phosphodiesterase-10A in the brain. J Nucl Med.